# ^64^Cu-Labeled cysteine–tagged epidermal growth factor

Chemical name: | ^64^Cu-Labeled cysteine–tagged epidermal growth factor
Abbreviated name: | [^64^Cu]Cys-EGF; EGF-PEG-DOTA/Cu
Synonym:
Agent Category: | Ligand
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the protein and nucleotide sequence (http://www.ncbi.nlm.nih.gov/nuccore/166362727?report=genbank) of human epidermal growth factor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=role+of+growth+factors+in+cancer)]

Growth factors such as the epidermal growth factor (EGF), the vascular endothelial growth factor (VEGF), and the tumor necrosis factor are known to have important roles in the development and progression of cancers (1-3). The EGF mediates its activity through a group of tyrosine kinase (TK)–dependent EGF receptors (EGFR) that promote not only cell proliferation but also cell survival and the motility phenotype that is necessary for the development of an invasive cancer (4). As a consequence, the EGFRs and their associated TKs are the targets of several anti-EGFR antibodies (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies) and TK inhibitors (http://clinicaltrials.gov/ct2/results?term=EGFR+tyrosine+kinase+inhibitors) that are either approved by the United Stated Food and Drug Administration or are being evaluated in clinical trials for the treatment of various neoplasms. Before treatment, the patients are screened to determine the extent of EGFR expression in the tumors with the use of immunohistochemistry (IHC) or fluorescence in situ hybridization (FISH) because these techniques help predict the probable therapeutic response and outcome for the individual (5, 6). However, only 10–25% of the patients who are EGFR-positive according to IHC or FISH analysis respond to the anti-EGFR therapy, which indicates that a poor correlation exists between the EGFR expression analysis and the treatment (7, 8). This is probably because only the active receptors are important to predict efficacy of the anti-EGFR agents for the treatment of cancers, and ICH and FISH do not distinguish between the active and inactive EGFR (9).

On binding the ligand, a characteristic feature of a functional EGFR is that it is internalized by the cell. Levashova et al. (10) envisioned that perhaps the natural ligand EGF itself could be used as an imaging agent to detect the active EGFRs in tumors. The investigators used an Escherichia coli (E. coli)–expressed EGF containing an N-terminal cysteine fusion tag of 15 amino acids (Cys-EGF) that can be used to conjugate therapeutic or imaging probes as done earlier with VEGF (11). In addition, because an active EGF/EGFR complex is composed of two molecules each of EGF and EGFR, the investigators also bioengineered an N-terminal cysteine fusion tag containing a dimeric EGF (dEGF) molecule, with the second EGF molecule linked to the first through a linker of 9 amino acids (11). The EGF and the dEGF were then labeled with radioactive copper (^64^Cu) to obtain [^64^Cu]Cys-EGF and [^64^Cu]Cys-dEGF. The biodistribution and imaging characteristics of the two molecules were then investigated in mice bearing xenograft tumors. It is pertinent to mention here that the imaging and biodistribution studies of only [^64^Cu]Cys-EGF are described in this chapter. Investigations performed with [^64^Cu]Cys-dEGF are described separately in MICAD (www.micad.nih.gov).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cys-tagged+EGF+synthesis)]

The Cys-EGF was expressed in and purified from E. coli as described elsewhere to obtain Cys-tagged single-chain VEGF (Cys-scVEGF) (12). Purified Cys-EGF was labeled with ^64^Cu as described elsewhere (12) with a procedure developed to label scVEGF using pegylated-1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (PEG-DOTA). The EGF-PEG-DOTA complex was purified with reverse-phase high-performance liquid chromatography, and purity of the product was reported to be >90% (10). Unconjugated ^64^Cu was removed by the addition of ethylenediamine tetraacetic acid, and the radiolabeled Cys-EGF (EGF-PEG-DOTA/Cu) was purified with size-exclusion chromatography on a NP-5 column (10). The radiochemical purity of EGF-PEG-DOTA/Cu was not reported. Specific activity of EGF-PEG-DOTA/Cu was reported to be ~4.6 MBq/μg (~125 μCi/μg) (10). The stability of EGF-PEG-DOTA/Cu was reported to be at least 3 h at room temperature in phosphate-buffered saline and at least 75 min at 37°C in plasma (10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+Cys-EGF+in+vitro)]

Using F98/EGFR(F) rat glioma cells that overexpress the human EGFR, the receptor affinity constant for EGF-PEG-DOTA/Cu was determined with Scatchard’s analysis to be 3.0 nM (10). In another study, EGF-PEG-DOTA was reported to induce EGFR TK phosphorylation in these cells in a dose-dependent manner (10). EGF-PEG-DOTA/Cu was also reported to compete with an EGF-Shiga-like toxin subunit A conjugate (EGF-SLT (http://www.sibtech.com/?p=targeted_toxins)) for binding to the EGFR (10). EGF-SLT is extremely toxic to MDA23 1luc human breast cancer cells, and the ability of proteins to compete for binding with the EGFR was measured by counting the number of cells surviving after a 72-h exposure to EGF-SLT (1 nM) in the presence of an increasing concentration of Cys-EGF (0–25 nM). It was reported that cell survival increased with an increasing EGF-PEG-DOTA/Cu concentration under these experimental conditions, which indicates that EGF-PEG-DOTA/Cu protected the cells from EGF-SLT toxicity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+rodentia)]

Levashova et al. studied the blood clearance and biodistribution of EGF-PEG-DOTA/Cu in mice (n = 4 animals) bearing F98/EGFR or MDA23 1luc cell tumors (10). The animals were injected with the radiotracer, and blood was collected at preselected time points for up to 60 min. More than 95% of the radioactivity was reported to clear from blood within 60 min. To determine biodistribution of the labeled protein, the animals were euthanized 3 h after administration of the tracer, all the major organs and tumors were harvested, and incorporated radioactivity in the harvested organs was counted using a gamma counter. The radioactivity was reported to accumulate primarily in the liver (~14.5% injected dose/gram tissue (% ID/g)) and kidneys (~10.5% ID/g). Also, the MDA23 1luc cell tumors were reported to have a higher accumulation of radioactivity than the F98/EGFR cell tumors although the former cells are known to express approximately five-fold less EGFR compared with the latter cells (10). The investigators suggested that this was probably because a higher number of functional receptors were present in the MDA23 1luc cells than in the F98/EGFR cells. No competition studies were reported.

The accumulation of EGF-PEG-DOTA/Cu was investigated in mice bearing orthotopic MDA23 1luc cell tumors (10). The animals (n = 4 mice per model) were injected with the radiolabeled protein and imaged 3 h later with positron emission tomography. The investigators observed selective radioactivity uptake by the tumors in the animals. No competition studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99m+Tc+Cys+EGF+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Wu W.K., Tse T.T., Sung J.J., Li Z.J., Yu L., Cho C.H. (2009). Expression of ErbB receptors and their cognate ligands in gastric and colon cancer cell lines. Anticancer Res.
2 Schoenleber S.J., Kurtz D.M., Talwalkar J.A., Roberts L.R., Gores G.J. (2009). Prognostic role of vascular endothelial growth factor in hepatocellular carcinoma: systematic review and meta-analysis. Br J Cancer.
3 Balkwill F. (2009). Tumour necrosis factor and cancer. Nat Rev Cancer.
4 Wilkins-Port C.E., Ye Q., Mazurkiewicz J.E., Higgins P.J. (2009). TGF-beta1 + EGF-initiated invasive potential in transformed human keratinocytes is coupled to a plasmin/MMP-10/MMP-1-dependent collagen remodeling axis: role for PAI-1. Cancer Res.
5 Baselga J., Arteaga C.L. (2005). Critical update and emerging trends in epidermal growth factor receptor targeting in cancer. J Clin Oncol.
6 Varella-Garcia M., Mitsudomi T., Yatabe Y., Kosaka T., Nakajima E., Xavier A.C., Skokan M., Zeng C., Franklin W.A., Bunn P.A., Hirsch F.R. (2009). EGFR and HER2 genomic gain in recurrent non-small cell lung cancer after surgery: impact on outcome to treatment with gefitinib and association with EGFR and KRAS mutations in a Japanese cohort. J Thorac Oncol.
7 Chung K.Y., Shia J., Kemeny N.E., Shah M., Schwartz G.K., Tse A., Hamilton A., Pan D., Schrag D., Schwartz L., Klimstra D.S., Fridman D., Kelsen D.P., Saltz L.B. (2005). Cetuximab shows activity in colorectal cancer patients with tumors that do not express the epidermal growth factor receptor by immunohistochemistry. J Clin Oncol.
8 Bell D.W., Lynch T.J., Haserlat S.M., Harris P.L., Okimoto R.A., Brannigan B.W., Sgroi D.C., Muir B., Riemenschneider M.J., Iacona R.B., Krebs A.D., Johnson D.H., Giaccone G., Herbst R.S., Manegold C., Fukuoka M., Kris M.G., Baselga J., Ochs J.S., Haber D.A. (2005). Epidermal growth factor receptor mutations and gene amplification in non-small-cell lung cancer: molecular analysis of the IDEAL/INTACT gefitinib trials. J Clin Oncol.
9 Johns T.G., Perera R.M., Vernes S.C., Vitali A.A., Cao D.X., Cavenee W.K., Scott A.M., Furnari F.B. (2007). The efficacy of epidermal growth factor receptor-specific antibodies against glioma xenografts is influenced by receptor levels, activation status, and heterodimerization. Clin Cancer Res.
10 Levashova Z., Backer M.V., Horng G., Felsher D., Backer J.M., Blankenberg F.G. (2009). SPECT and PET imaging of EGF receptors with site-specifically labeled EGF and dimeric EGF. Bioconjug Chem.
11 Levashova Z., Backer M., Backer J.M., Blankenberg F.G. (2008). Direct site-specific labeling of the Cys-tag moiety in scVEGF with technetium 99m. Bioconjug Chem.
12 Backer M.V., Levashova Z., Patel V., Jehning B.T., Claffey K., Blankenberg F.G., Backer J.M. (2007). Molecular imaging of VEGF receptors in angiogenic vasculature with single-chain VEGF-based probes. Nat Med.